# Glycol chitosan/heparin-immobilized gold-deposited iron oxide nanoparticles

Chemical name: | Glycol chitosan/heparin-immobilized gold-deposited iron oxide nanoparticles
Abbreviated name: | Composite NPs
Synonym:
Agent Category: | Nanoparticles
Target: | Fibrinogen-derived product in tumor stroma
Target Category: | Adhesion molecules
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=tumor%20stroma%20and%20clotted%20plasma)]

Glycol chitosan/heparin-immobilized gold-deposited iron oxide (IO) nanoparticles (NPs), abbreviated as composite NPs, are a NP-based contrast agent developed by Yuk et al. for tumor stroma-targeted magnetic resonance imaging (MRI) (1).

Tumor tissue is different from normal tissue in the content and function of its stroma. At the initial stage of tumor development, tumor cells secrete growth factors, including vascular permeability factor that renders the local microvasculature hyperpermeable to fibrinogen and other plasma proteins. Extravasated fibrinogen crosslinks with fibrin and other proteins, forming a meshwork in the tumor stroma (2, 3). This sequence also occurs in the process of wound-healing and in the progression of many other diseases, but the tumor stroma contains increased amounts of fibrinogen, collagen, fibronectin, fibrinogen-derived products, and other proteins (2, 4). These proteins either come from the leaky blood vessels or are inappropriately synthesized by the tumor cells. Functionally, normal stroma generates an antiproliferative environment, whereas tumor stroma promotes tumor cell proliferation, migration, and lymphovascular invasion by providing adhesion proteins, proteases, and growth factors (5).

Abnormal formation of clotted plasma protein meshwork in the tumor stroma and on the tumor blood vessel walls has prompted investigators to generate tumor stroma-targeted imaging and therapeutic agents. Pilch et al. screened a phage library on plasma clots and obtained two cyclic decapeptides (CLT; CLT1 and CLT2) (3). The fluorescence-labeled CLT peptides specifically accumulated in the fibrillar meshwork that existed in tumor stroma, but they were not detectable in other tissues in animal models of human tumors. Ye et al. conjugated the CLT1 peptide with gadolinium-diethylenetriamine pentaacetic acid (Gd-DTPA), and the generated agent Gd-DTPA-CLT1 (http://www.ncbi.nlm.nih.gov/books/NBK23114/#Gd-DTPA-CLT1.Background) exhibited high specificity to the fibronectin-fibrin complexes in the tumor stroma (6). Simberg et al. also reported the clotted plasma protein-targeted multimodal agent CREKA-SPIO-Cy7 (http://www.ncbi.nlm.nih.gov/books/NBK23725/#CREKA-SPIO.Background), which was synthesized by conjugation of the peptide CREKA with superparamagnetic IO and cyanine 7 (7). On the basis of the interaction between the fibrinogen-derived products and heparin, Yuk et al. synthesized the MRI contrast agent composite NPs with heparin as the specific ligand (1). Heparin is a highly-sulfated glycosaminoglycan with a high negative charge density. Heparin has two commercial types: unfractionated heparin (UFH, 12–15 kDa) and low molecular weight heparin (LMWH, 2–9 kDa) (8). UFH is a heterogeneous mixture of glycosaminoglycans that bind to the enzyme inhibitor antithrombin III via the pentasaccharide. UFH also binds many other proteins, endothelial cells, platelets, and other circulating cells. LMWH is produced by the depolymerization of heparin and acts by targeting factor Xa activity, rather than by activating anti-thrombin activity. Heparin also exhibits anti-tumor effects by inhibiting tumor growth and spread. Composite NPs have been shown to selectively distribute in tumors in an animal model of murine squamous cell carcinoma (SCC). This chapter summarizes the data obtained with the composite NPs (1).

### Related Resource Links:

Tumor stroma clotted plasma protein-targ (http://www.ncbi.nlm.nih.gov/books/?term=tumor%20stroma%20and%20clotted%20AND%20micad%5bbook%5d) e (http://www.ncbi.nlm.nih.gov/books/?term=tumor%20stroma%20and%20clotted%20AND%20micad%5bbook%5d) ted imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=tumor%20stroma%20and%20clotted%20AND%20micad%5bbook%5d)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21506550)]

Yuk et al. synthesized the composite NPs on the basis of ionic interactions among the following components: IO nanoseeds, gold, glycol chitosan (carrier), and heparin (specific ligand) (1). IO nanoseeds and glycol chitosan are cationic while gold and heparin are anionic in aqueous solution.

The yield of IO nanoseeds increased with increased reaction temperature, and the IO nanoseeds formed at 80°C were used throughout the study. To induce the interaction between IO nanoseeds and glycol chitosan, gold was first deposited on the surface of IO nanoseeds to induce an anionic charge on the NP surface. The formation of gold on the IO nanoseeds was induced as a function of added volume of 1 mM HAuCl_4_ in aqueous solution. The amounts of Fe and gold in the gold-deposited IO NPs used for studies were 99.83 wt. % and 0.17 wt. %, respectively. The gold-deposited IO NPs were then embedded into the cationic glycol chitosan matrix. The gold-deposited IO/glycol chitosan NPs were subsequently immobilized with negatively charged heparin to generate the imaging agent, composite NPs. Composite NPs were freeze-dried in the pluronic F-68 aqueous solution. During the process, pluronic F-68 was adsorbed onto the composite NPs, which avoided the aggregation and improved the stability of the composite NPs in the aqueous media. To visualize the tumor-targeting of the composite NPs in vivo, the composite NPs and the intermediates were also labeled with cyanine 5.5 (Cy5.5). The content of Cy5.5 molecules was fixed to 1% of the composite NPs (weight).

The diameters of the composite NPs and lyophilized composite NPs were determined to be ~118.4 nm and 134.8 nm, respectively. The content (%) of metal NPs and zeta potential were 3.57 wt. % and 12.48 mV for the composite NPs, 2.40 wt. % and 5.67 mV for the lyophilized composite NPs, respectively. The composite NPs did not show aggregation within 5 days in phosphate-buffered saline, but disintegration of the composite NPs was observed with leakage and aggregation of the gold-deposited IO NPs over time. With phantoms containing same concentrations of composite NPs and commercial contrast agent Resovist, T2*-weighted images showed that the composite NPs generated stronger signal enhancement and exhibited higher magnetic properties than Resovist.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21506550)]

The cytotoxicities of the IO nanoseeds, gold-deposited IO NPs, and gold-deposited IO/glycol chitosan NPs with or without heparin were evaluated with cultured murine SCC-7 cells (1). All the samples exhibited dose-dependent cytotoxicity, showing decreased cell viability. However, the composite NPs were less cytotoxic than the IO nanoseeds and the gold-deposited IO NPs (P < 0.05). The 50% inhibitory concentrations of IO nanoseeds, gold-deposited IO NPs, gold-deposited IO/glycol chitosan NPs, and composite NPs were 18.96, 14.6, 34.96, and 24.71 mg/ml, respectively. No binding studies were carried out to show the specificity of the composite NPs.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21506550)]

Optical imaging and MRI were performed in male C3H/HeN mice bearing SCC-7 tumors (1). The number of animals used for imaging was not described.

Optical imaging showed strong fluorescence in the tumor at 1 h after injection of Cy5.5-labeled composite NPs. The fluorescence reached a maximum at 9 h and was still detectable for >48 h. Only a weak fluorescent signal was observed in the tumors from the mice injected with Cy5.5-labeled composite NPs without heparin or with free Cy5.5.

MRI showed that the composite NPs produced stronger enhancement of the tumor than the composite NPs without heparin and Resovist during the imaging period (1–6 h after injection).

Histological studies of the tumor tissue obtained at 12 h after injection confirmed the accumulation of the composite NPs with hemotoxylin and eosin staining and Prussian blue staining. Blocking studies were not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Yuk S.H., Oh K.S., Cho S.H., Lee B.S., Kim S.Y., Kwak B.K., Kim K., Kwon I.C. (2011). Glycol chitosan/heparin immobilized iron oxide nanoparticles with a tumor-targeting characteristic for magnetic resonance imaging. Biomacromolecules.
2 Simpson-Haidaris P.J., Rybarczyk B. (2001). Tumors and fibrinogen. The role of fibrinogen as an extracellular matrix protein. Ann N Y Acad Sci.
3 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
4 Rybarczyk B.J., Lawrence S.O., Simpson-Haidaris P.J. (2003). Matrix-fibrinogen enhances wound closure by increasing both cell proliferation and migration. Blood.
5 Malik G., Knowles L.M., Dhir R., Xu S., Yang S., Ruoslahti E., Pilch J. (2010). Plasma fibronectin promotes lung metastasis by contributions to fibrin clots and tumor cell invasion. Cancer Res.
6 Ye F., Wu X., Jeong E.K., Jia Z., Yang T., Parker D., Lu Z.R. (2008). A peptide targeted contrast agent specific to fibrin-fibronectin complexes for cancer molecular imaging with MRI. Bioconjug Chem.
7 Simberg D., Duza T., Park J.H., Essler M., Pilch J., Zhang L., Derfus A.M., Yang M., Hoffman R.M., Bhatia S., Sailor M.J., Ruoslahti E. (2007). Biomimetic amplification of nanoparticle homing to tumors. Proc Natl Acad Sci U S A.
8 Norrby K. (2006). Low-molecular-weight heparins and angiogenesis. APMIS.